# ^99m^Tc-Tricarbonyl-K-H-K-H-cholecystokinin 8

Chemical name: | ^99m^Tc-Tricarbonyl-K-H-K-H-cholecystokinin 8
Abbreviated name: | [^99m^Tc](KH)_2_CCK8
Synonym:
Agent Category: | Peptide
Target: | Cholecystokinin receptor 2 (CCK2R)
Target Category: | Receptor-ligand binding
Method of detection: | Single-photon emission computed tomography (SPECT); planar gamma imaging
Source of Signal/Contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click here for protein and nucleotide (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=retrieve&dopt=full_report&list_uids=886&log$=databasead&logdbfrom=protein) information regarding cholecystokinin A receptor

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CCK8%5BAll+Fields%5D)]

Cholecystokinin (CCK) is a peptide hormone that has an important role in the digestion of food because it stimulates contraction of the gallbladder and pancreatic enzyme secretion, and in the presence of secretin it enhances blood flow and bicarbonate secretion from the pancreas (1). CCK is produced and released by cells of the duodenum and the jejunum in response to a variety of peptides, amino acids, and fatty acids, but not carbohydrates. In addition to its activity in the gut, CCK is also known to act as a neurotransmitter in the brain (2). Mouse and human CCK genes show a very high homology (>70%) and act through two receptors designated as CCK-AR (or CCK1R) and CCK-BR (or CCK2R); under physiological conditions CCK acts primarily through the CCK-AR (3). Pancreatic secretions have also been shown to be mediated by CCK through the indirect cholinergic vagal innervations pathway, which indicates that CCK receptors are also present on vagal neurons (4). Although the original CCK molecule was purified as a peptide (33 amino acids) from porcine intestine, several forms of the peptide including CCK58, CCK39, CCK33, CCK22, and CCK8 have been isolated from the intestines of various animals. Among these CCK peptide forms, the C-terminal heptapeptide possesses the complete spectrum of activities attributed to the parent molecule (1). The long forms of the molecule are known to have a longer circulation half-life compared with the shorter molecules, and they also show some differences in their biological activities (5, 6). A splice variant of the CCK-BR that was identified in colorectal and pancreatic cancer tissue was shown to bind CCK8 and other related peptides such as gastrin (7). The United States Food and Drug Administration (FDA) has approved several clinical trials (http://clinicaltrials.gov/ct2/results?term=Cholecystokinin+) involving CCK for the treatment of different gastrointestinal disorders such as bulimia nervosa, chronic pancreatitis, and binge eating.

The field of receptors has received a great deal of attention because of its involvement in a variety of cancers, and the development of antibodies and peptides that show high binding specificity for the receptors has encouraged investigators to use receptor imaging techniques to detect and diagnose the different diseases as well as to devise appropriate treatments (8-10). The use of peptides for imaging has certain advantages over the use of intact proteins (e.g., antibodies) because peptides are easy (and relatively inexpensive) to synthesize, show high receptor affinity and specificity, usually have fast clearance from circulation, and produce a high tumor/normal tissue signal ratio (8, 11). Because of their superior performance over intact proteins or antibodies, somatostatin-based peptides such as octreotide labeled with radioactive indium or technetium (^99m^Tc), along with other peptides, have been approved by the FDA and are widely used for the imaging of cancers (12, 13). D’Andrea et al. synthesized a CCK8 derivative with a histidine chelator labeled with ^99m^Tc and evaluated its in vitro characteristics and biodistribution in nude mice bearing xenograft tumors generated with A431 (http://www.biocompare.com/itemdetails.asp?itemid=348853) human squamous carcinoma cells transfected with CCK2R (14, 15).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CCK8+(99m)Tc+tricarbonyl+synthesis)](15)

Synthesis of the CCK8 derivative was described by D’Andrea et al. (15). Briefly, the peptide was synthesized on an ABI 433 peptide synthesizer with solid-phase rink-amide MBHA resin and N-(9-fluorenyl)methoxycarbonyl (Fmoc) chemistry. For selective deprotection, the lysine residues were protected with a methyltrytil group. After selective deprotection and neutralization with N,N-diisopropylethylamine in dimethyl formamide, the generated Fmoc-histidine(Trt)-OH (http://www.chemimpex.com/product1.asp?p=02874) was coupled to the resin, and the Fmoc was cleaved (15). This reaction produced a crude (KH)_2_-CCK8 peptide that was precipitated with ethyl ether and freeze-dried. The peptide was purified with high-performance liquid chromatography (HPLC) on a C_18_ column, and its purity was determined with HPLC and matrix-assisted laser desorption/ionization-time of flight mass spectrometry. The yields and purity of the intermediate compounds and the final product obtained from the various synthesis reactions and purification procedures were not reported (15).

To label (KH)_2_-CCK8 with ^99m^Tc, the carbonyl complex of ^99m^Tc ([^99m^Tc(OH_2_)_3_(CO)_3_]^+^) was prepared with a commercial kit according the manufacturer’s instructions (15). An aliquot of the carbonyl complex was incubated with (KH)_2_-CCK8 at room temperature (duration was not reported), and formation of the radioactive compound ([^99m^Tc(CO)_3_](KH)_2_-CCK8) was verified with HPLC. The radiolabeled peptide was reported to have a specific activity of 1,850–3,700 GBq/mmol (50–100 Ci/mmol). Stability of the labeled compound was investigated under in vivo conditions, and several breakdown products were reported as determined with HPLC analysis of the blood (15).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+carbonyl+CCK8+in+vitro)]

The binding affinity of [^99m^Tc(CO)_3_](KH)_2_-CCK8 was determined using serial dilutions of the compound (0.05–120 nM) with A431 cells overexpressing the CCK2R in culture medium at 4°C for 1 h (15). Non-specific binding was assessed in the presence of 100- to 1,000-fold excess of unlabeled peptide. The binding was terminated by washing the cells twice with phosphate-buffered saline (PBS), and the cells were solubilized with 0.1 N sodium hydroxide. The radioactivity was counted in a gamma counter, and the amount recovered was normalized for protein content. Internalization of the compound was determined by comparing the difference in incorporated radioactivity in equal numbers of cells incubated with the radioactive compound for 60 and 120 min at 4°C and 37°C, respectively. The cells were subsequently washed with PBS to remove all unbound radioactivity and incubated with 30 μM unlabeled [Tc(CO)_3_](KH)_2_-CCK8 at 4°C to displace any surface-bound radioactivity. Bound label was determined and normalized as mentioned above. The peptide was determined to have a dissociation equilibrium constant of ~30 nM with an apparent receptor number (maximal binding) of 5.8 pmol/mg protein. A progressive internalization of the peptide by the cells was observed only at 37°C; at 4°C the radioactivity was reported to remain constant at 60 and 120 min after exposure to the labeled compound indicating an active process.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+carbonyl+CCK8+rodentia)]

The in vivo biodistribution of [^99m^Tc(CO)_3_](KH)_2_-CCK8 was studied in nude mice bearing A431-CCK2R cell xenograft tumors (15). For controls, mice with A431 cell xenograft tumors were used. The labeled peptide was injected into the lateral tail vein, and the animals (n = at least 5 mice per time point) were killed 30 and 120 min after the injection. Various organs were harvested from the animals, and accumulated radioactivity was measured in a gamma counter. The uptake of [^99m^Tc(CO)_3_](KH)_2_-CCK8 was reported to be higher in the A431-CCK2R cell tumors compared with the controls in a ratio of 2.3:1 at 120 min after administration of radioactivity. The kidneys showed the highest retention of the label (7.35% injected dose/g tissue (% ID/g)) at 120 min, and the liver had accumulated close to 4% ID/g at this time point. All other organs had <4% ID/g of the radiochemical at 120 min. The radioactivity was cleared rapidly from blood circulation with only 0.75% ID/g remaining in this tissue at 120 min. Gamma imaging of the animals 120 min after administration of [^99m^Tc(CO)_3_](KH)_2_-CCK8 showed high background radioactivity in the kidneys, liver, and the gastrointestinal tract, as observed during the tissue biodistribution studies.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+carbonyl+CCK8+non+primate+mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+carbonyl+CCK8+non+human+primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+carbonyl+CCK8+humans)]

No references are currently available.

## Supplemental Information

[Disclaimers]

## References

1 Green G.M., Reeve J.R. (2008). Unique activities of cholecystokinin-58; physiological and pathological relevance. Curr Opin Endocrinol Diabetes Obes.
2 Saluja A., Logsdon C., Garg P. (2008). Direct Versus Indirect Action of Cholecystokinin on Human Pancreatic Acinar Cells: Is It Time for a Judgment after a Century of Trial?. Gastroenterology.
3 Wank S.A., Pisegna J.R., de Weerth A. (1994). Cholecystokinin receptor family. Molecular cloning, structure, and functional expression in rat, guinea pig, and human. Ann N Y Acad Sci.
4 Weiss F.U., Halangk W., Lerch M.M. (2008). New advances in pancreatic cell physiology and pathophysiology. Best Pract Res Clin Gastroenterol.
5 Eysselein V.E., Bottcher W., Kauffman G.L., Walsh J.H. (1984). Molecular heterogeneity of canine cholecystokinin in portal and peripheral plasma. Regul Pept.
6 Reeve J.R., McVey D.C., Bunnett N.W., Solomon T.E., Keire D.A., Ho F.J., Davis M.T., Lee T.D., Shively J.E., Vigna S.R. (2002). Differences in receptor binding and stability to enzymatic digestion between CCK-8 and CCK-58. Pancreas.
7 Laverman P., Roosenburg S., Gotthardt M., Park J., Oyen W.J., de Jong M., Hellmich M.R., Rutjes F.P., van Delft F.L., Boerman O.C. (2008). Targeting of a CCK(2) receptor splice variant with (111)In-labelled cholecystokinin-8 (CCK8) and (111)In-labelled minigastrin. Eur J Nucl Med Mol Imaging.
8 Abraham J.M., Cheng Y., Hamilton J.P., Paun B., Jin Z., Agarwal R., Kan T., David S., Olaru A., Yang J., Ito T., Selaru F.M., Mori Y., Meltzer S.J. (2008). Generation of small 32P-labeled peptides as a potential approach to colorectal cancer therapy. PLoS ONE.
9 Sandstrom K., Nestor M., Ekberg T., Engstrom M., Anniko M., Lundqvist H. (2008). Targeting CD44v6 Expressed in Head and Neck Squamous Cell Carcinoma: Preclinical Characterization of an In-Labeled Monoclonal Antibody. Tumour Biol.
10 Migliore A., Signore A., Capuano A., Bizzi E., Massafra U., Vacca E., Todino V., Chianelli M. (2008). Relevance of 99mTc-HYNIC-tir-octreotide scintigraphy in a patient affected by sarcoidosis with lung and joints involvement and secondary Sjogren's syndrome treated with infliximab: case report. Eur Rev Med Pharmacol Sci.
11 Stewart K.M., Horton K.L., Kelley S.O. (2008). Cell-penetrating peptides as delivery vehicles for biology and medicine. Org Biomol Chem.
12 Heppeler A., Froidevaux S., Eberle A.N., Maecke H.R. (2000). Receptor targeting for tumor localisation and therapy with radiopeptides. Curr Med Chem.
13 Dijkgraaf I., Boerman O.C., Oyen W.J., Corstens F.H., Gotthardt M. (2007). Development and application of peptide-based radiopharmaceuticals. Anticancer Agents Med Chem.
14 Aloj L., Caraco C., Panico M., Zannetti A., Del Vecchio S., Tesauro D., De Luca S., Arra C., Pedone C., Morelli G., Salvatore M. (2004). In vitro and in vivo evaluation of 111In-DTPAGlu-G-CCK8 for cholecystokinin-B receptor imaging. J Nucl Med.
15 D'Andrea L.D., Testa I., Panico M., Stasi R.D., Caraco C., Tarallo L., Arra C., Barbieri A., Romanelli A., Aloj L. (2008). In vivo and in vitro characterization of CCK8 bearing a histidine-based chelator labeled with (99m)Tc-tricarbonyl. Biopolymers.